# [^125^I]-Labeled monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII)

Chemical name: | [^125^I]-Labeled monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII)
Abbreviated name: | [^125^I]SGMIB-L8A4
Synonym:
Agent Category: | Monoclonal antibody
Target: | Epidermal growth factor receptor variant III (EGFRvIII)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography; gamma planar imaging
Source of signal / contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ch806&cmd=DetailsSearch)]

The biological characteristics, activating ligands, functions, and signal transduction pathways of the various transmembrane epidermal growth factor receptors (EGFRs) are described elsewhere (1-3). The EGFRs are known to regulate the growth, survival, differentiation, and migration of cells through the activation of an associated intracellular tyrosine kinase (TK) signaling pathway, and they are overexpressed in many malignant epithelial tumors (2, 3). Overexpression of the EGFR in tumors has been attributed to cellular amplification of the receptor gene, and this phenomenon may result in the production of a mutated receptor in the cell (2, 4). In addition, overexpression of the EGFR in tumors usually indicates a poor clinical prognosis for a cancer patient (4). The most common mutation observed in the receptor is the deletion of an extracellular domain segment of the EGFR, including the ligand-binding region, and this generates a variant known as EGFRvIII or de2-7 EGFR (2, 4). The generation, structure, functions, and role of EGFRvIII in tumor malignancy was reviewed by Gan et al. (5). Although EGFRvIII is nonresponsive to a ligand due to the absence of a ligand-binding site, it is constitutively active with a constantly operating downstream TK signal transduction pathway that appears to promote the development of a neoplastic phenotype, particularly for glioblastoma and to some extent for other cancers such as those of the prostate and the breast (2, 6).

Because the EGFR promotes and helps maintain transformed cells, several anti-EGFR antibodies (http://google2.fda.gov/search?q=anti-EGFR+antibodies+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=6) that inhibit the activity of this receptor and small molecule drugs (http://google2.fda.gov/search?q=EGFR+Tyrosine+kinase+inhibitor&spell=1&client=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&ie=UTF-8&site=FDAgov&access=p) that block the downstream TK signaling pathway were developed and have been approved by the United States Food and Drug Administration for the treatment of certain cancers (2). The antibodies are designed to target the extracellular domain of the receptor, block ligand binding, and inhibit activation of the TK signal transduction pathway, which leads to downregulation of the EGFR on the cell surface. However, because EGFRvIII lacks the ligand-binding region on the extracellular domain, these antibodies cannot obstruct the constitutive mutant receptor activity (2). Hence, a monoclonal antibody (mAb), designated mAb806 and specifically targets the EGFRvIII, was generated and has been characterized in preclinical studies (7, 8). Subsequently, a chimeric form of the mAb (chAb), designated ch806, was developed and evaluated in a phase I clinical trial involving patients with cancerous tumors that overexpressed the EGFRvIII. Results from this trial indicated that ch806 could be a suitable biotherapeutic agent to treat cancers (4). Various studies performed with mAb806 or ch806 are described in separate chapters of MICAD (http://www.ncbi.nlm.nih.gov/books/?term=ch806%20AND%20micad%5Bbook%5D).

Studies are also in progress with another anti-EGFRvIII mAb, L8A4, to develop a radioimmunotherapeutic (RIT) agent for the treatment of cancer (9, 10). In a recent study, the use of acyclic ([(R)-2-amino-3-(4-isothiocyanatophenyl)propyl]-trans-(S,S)-cyclohexane-1,2-diamine-pentaacetic acid (CHX-A''-DTPA) and 2-(4-isothiocyanatobenzyl)-6-methyldiethylene-triaminepentaacetic acid (1B4M-DTPA) as well as the macrocyclic ligands (S)-2-(4-isothiocyanatobenzyl)-1,4,7,10-tetraazacyclododecane-tetraacetic acid (C-DOTA) and α-(5-isothiocyanato-2-methoxyphenyl)-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (MeO-DOTA) was evaluated for the labeling of L8A4 with ^177^Lu, which was considered suitable to generate an RIT agent against cancer (10). The characteristics of the various ^177^Lu-labeled conjugates of L8A4 ([^177^Lu]-CHX-A''-DTPA-L8A4, [^177^Lu]-1B4M-DTPA-L8A4, [^177^Lu]-C-DOTA-L8A4, and [^177^Lu]-MeO-DOTA-L8A4) were compared to the characteristics of L8A4 labeled with N-succinimidyl 4-guanidinomethyl-3-[^125^I]iodobenzoate ([^125^I]SGMIB-L8A4) under in vitro (9) and in vivo (10) conditions.

This chapter describes results obtained from the in vitro and the biodistribution studies performed with [^125^I]SGMIB-L8A4 in athymic mice bearing subcutaneous U87MG.∆EGFR cell glioma xenograft tumors. Results obtained with [^177^Lu]-CHX-A''-DTPA-L8A4, [^177^Lu]-1B4M-DTPA-L8A4, [^177^Lu]-C-DOTA-L8A4, and [^177^Lu]-MeO-DOTA-L8A4 are presented in separate chapters of MICAD (www.micad.nih.gov) (11-14).

### Other Sources of Information

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_005228.3) of human EGFR variant 1

EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim/131550) (Online Mendelian Inheritance in Man)

EGFR signaling pathways (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=200086&source=NATURE&what=graphic&jpg=on) (NCI-Nature Pathways Interaction Database)

Anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-EGFR%20antibodies&cmd=DetailsSearch) in PubMed

EGFR tyrosine kinase inhibitors (http://www.ncbi.nlm.nih.gov/pubmed?term=egfr%20tyrosine%20kinase%20inhibitors&cmd=DetailsSearch) in PubMed

Chapters on anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

Other chapters on anti-EGFRvIII antibodies (http://www.ncbi.nlm.nih.gov/books/?term=EGFRvIII%20AND%20micad%5Bbook%5D) in MICAD

Clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFRvIII+) with EGFRvIII as a target

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Synthesis%20of%20L8A4%20antibody&cmd=DetailsSearch)]

The preparation, purification, characterization, conjugation with the various metal chelating agents, and radiolabeling of L8A4 with ^125^I (using N-succinimidyl 4-guanidinomethyl-3-[^125^I]iodobenzoate ([^125^I]SGMIB)) are discussed by Hens et al. (10). The specific activity of [^125^I]SGMIB-L8A4 used in the various studies was reported to vary from 0.111–0.185 MBq/6.6 pmol (3–5 μCi/6.6 pmol) to 0.026–0.118 MBq/6.6 pmol (0.7–3.2 μCi/6.6 pmol). The radiochemical yield and purity of the labeled mAb were not reported. However, the labeled mAb was shown to elute as a single peak when analyzed with size-exclusion high-performance liquid chromatography, and the agent had a retention time that was similar to the native L8A4 mAb.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20in%20vitro%20studies&cmd=DetailsSearch)]

Using a magnetic bead assay, the immunoreactive fraction of [^125^I]SGMIB-L8A4 was determined to be 0% to 71% (9). A cell internalization assay with U87MG.∆EGFR cells showed that internalization of the ^125^I-labeled mAb peaked at 1 h after exposure to the tracer and was ~10% of the original cell-bound radioactivity. By 24 h after exposure, the internalization of radioactivity had gradually reduced to ~1% of the original value.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^125^I]SGMIB-L8A4 was studied in the major organs of athymic mice (n = 5 animals/group) bearing subcutaneous U87MG.∆EGFR cell glioma xenograft tumors (10). Data obtained from four independent studies at 1, 4, and 8 days postinjection (p.i.) of the labeled mAb are presented as percent of injected dose per gram tissue (% ID/g). Because the biodistribution trend of the radioiodinated mAb was the same in all of the studies, data discussed here are from only one such investigation (see Table 1 in Hens et al. (10)). The amount of radioactivity in the blood at 1 day p.i. was 18.78 ± 2.24% ID/g and decreased to 1.29 ± 0.87% ID/g by 8 days p.i. At 1 day p.i., the liver, kidneys, spleen, and lungs exhibited accumulation between 5% and 7% ID/g and the amount of label in all these organs decreased to ~0.5% ID/g by 8 days p.i. The amount of tracer accumulated in the muscles and bones was ~1.5 and ~3.5% ID/g, respectively, at 1 day p.i.; by 8 days p.i., accumulation decreased to ~0.15% ID/g and ~0.33% ID/g, respectively, in these tissues. The tumor had a radioactivity accumulation of 21.64 ± 4.53% ID/g at 1 day p.i., which decreased to 2.86 ± 0.98% ID/g by 8 days p.i. The tumor/normal tissue ratios for liver, kidneys, spleen, lungs, muscles, and bone were reported to be 10.4 ± 2.6, 11.0 ± 2.4, 14.9 ± 3.9, 7.6 ± 2.5, 21.4 ± 6.9, and 15.4 ± 4.0, respectively at 3 days p.i. (for details see Table 5 in Hens et al. (10)). These results (summarized in Table 1 below) indicate that [^125^I]SGMIB-L8A4 is a suitable agent for the detection of tumors expressing EGFRvIII in rodents.

Table 1: Summary of tumor/normal tissue radioactivity uptake ratios for various organs obtained 3 days after the [^125^I]SGMIB-L8A4 injection. Data obtained from Table 5 in Hens et al. (10).

Conjugated mAb | Liver | Kidney | Spleen | Lungs | Muscles | Brain | Bone
[ ^ 125 ^ I]SGMIB-L8A4 | 10.4 ± 2.6 | 11.0 ± 2.4 | 14.9 ± 3.9 | 7.6 ± 2.5 | 21.4 ± 6.9 | 88.8 ± 17.4 | 15.4 ± 4.0

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L8A4%20antibody%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

These studies were supported by National Institutes of Health grants NS20023 and CA42324.

## References

1 Hasselbalch B., Lassen U., Poulsen H.S., Stockhausen M.T. (2010). Cetuximab insufficiently inhibits glioma cell growth due to persistent EGFR downstream signaling. Cancer Invest.
2 Pines G., Kostler W.J., Yarden Y. (2010). Oncogenic mutant forms of EGFR: lessons in signal transduction and targets for cancer therapy. FEBS Lett.
3 Spector N.L., Blackwell K.L. (2009). Understanding the mechanisms behind trastuzumab therapy for human epidermal growth factor receptor 2-positive breast cancer. J Clin Oncol.
4 Scott A.M., Lee F.T., Tebbutt N., Herbertson R., Gill S.S., Liu Z., Skrinos E., Murone C., Saunder T.H., Chappell B., Papenfuss A.T., Poon A.M., Hopkins W., Smyth F.E., MacGregor D., Cher L.M., Jungbluth A.A., Ritter G., Brechbiel M.W., Murphy R., Burgess A.W., Hoffman E.W., Johns T.G., Old L.J. (2007). A phase I clinical trial with monoclonal antibody ch806 targeting transitional state and mutant epidermal growth factor receptors. Proc Natl Acad Sci U S A.
5 Gan H.K., Kaye A.H., Luwor R.B. (2009). The EGFRvIII variant in glioblastoma multiforme. J Clin Neurosci.
6 Lee F.T., O'Keefe G.J., Gan H.K., Mountain A.J., Jones G.R., Saunder T.H., Sagona J., Rigopoulos A., Smyth F.E., Johns T.G., Govindan S.V., Goldenberg D.M., Old L.J., Scott A.M. (2010). Immuno-PET quantitation of de2-7 epidermal growth factor receptor expression in glioma using 124I-IMP-R4-labeled antibody ch806. J Nucl Med.
7 Jungbluth A.A., Stockert E., Huang H.J., Collins V.P., Coplan K., Iversen K., Kolb D., Johns T.J., Scott A.M., Gullick W.J., Ritter G., Cohen L., Scanlan M.J., Cavenee W.K., Old L.J. (2003). A monoclonal antibody recognizing human cancers with amplification/overexpression of the human epidermal growth factor receptor. Proc Natl Acad Sci U S A.
8 Perera R.M., Zoncu R., Johns T.G., Pypaert M., Lee F.T., Mellman I., Old L.J., Toomre D.K., Scott A.M. (2007). Internalization, intracellular trafficking, and biodistribution of monoclonal antibody 806: a novel anti-epidermal growth factor receptor antibody. Neoplasia.
9 Hens M., Vaidyanathan G., Welsh P., Zalutsky M.R. (2009). Labeling internalizing anti-epidermal growth factor receptor variant III monoclonal antibody with (177)Lu: in vitro comparison of acyclic and macrocyclic ligands. Nucl Med Biol.
10 Hens M., Vaidyanathan G., Zhao X.G., Bigner D.D., Zalutsky M.R. (2010). Anti-EGFRvIII monoclonal antibody armed with 177Lu: in vivo comparison of macrocyclic and acyclic ligands. Nucl Med Biol.
11 Chopra, A., 177Lu-Labeled [(R)-2-amino-3-(4-isothiocyanatophenyl)propyl]-trans-(S,S)-cyclohexane-1,2-diamine-pentaacetic acid (CHX-A″-DTPA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
12 Chopra, A., 177Lu-Labeled 2-(4-isothiocyanatobenzyl)-6-methyldiethylene-triaminepentaacetic acid (1B4M-DTPA)) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
13 Chopra, A., 177Lu-Labeled (S-2-(4-isothiocyanatobenzyl)-1,4,7,10-tetraazacyclododecane-tetraacetic acid (C-DOTA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
14 Chopra, A., 177Lu-Labeled α-(5-isothiocyanato-2-methoxyphenyl)-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (MeO-DOTA) conjugated monoclonal antibody L8A4 against epidermal growth factor receptor variant III (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.